# 1-(4-[^18^F]Fluoromethoxy-3-methoxyphenethyl)-4-(3-phenylpropyl)piperazine

Chemical name: | 1-(4-[^18^F]Fluoromethoxy-3-methoxyphenethyl)-4-(3-phenylpropyl)piperazine
Abbreviated name: | [^18^F]FM-SA4503
Synonym: | [^18^F]Fluoromethyl SA4503
Agent Category: | Compound
Target: | Sigma-one (σ_1_) receptor
Target Category: | Receptor binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5B18F%5DSA4503+OR+(fluorine-18-labeled+SA4503))]

1-(4-[^18^F]Fluoromethoxy-3-methoxyphenethyl)-4-(3-phenylpropyl)piperazine ([^18^F]FM-SA4503) is a radioligand developed for positron emission tomography (PET) imaging of the sigma (σ) receptors (1). It is a potent σ_1_ receptor agonist labeled with ^18^F, a positron emitter with a physical half-life (t_½_) of 109.8 min.

The σ receptors are functional, membrane-bound proteins distributed in the central nervous system (CNS) and peripheral organs (2). The CNS σ receptors are unique binding sites related to higher brain functions (3). They are distinct from opiate and phencyclidine binding sites. There are at least two subtypes of σ receptors: σ_1_ and σ_2_ receptors. The precise mechanism of the functional response of these receptors is not entirely known. These receptors appear to be involved in numerous pharmacological and physiological functions, and they also modulate a number of central neurotransmitter systems, including noradrenergic, glutamatergic, and dopaminergic systems. Phencyclidine and derivatives, cocaine and derivatives, some neuroleptics, atypical antipsychotic agents, and other chemically unrelated compounds can bind to the σ receptor sites. Studies have shown that these receptors may play a role in the pathogenesis of psychiatric disorders (4, 5). The σ_1_ receptor subtypes appear to play a role in motor function and potassium channels (2). The σ_2_ receptor subtypes are implicated in CNS disorders and malignant neoplastic diseases. Because of these effects, σ receptor ligands may be useful for detection and treatment in neurology and oncology.

Matsuno et al. (6) developed 1-(3,4-dimethoxyphenethyl)-4-(3-phenylpropyl)-piperazine dihydrochloride (SA4503), a potent σ_1_ agonist that is in phase II clinical trials as a therapeutic agent for functional recovery after stroke. SA4503 is highly selective for σ_1_ receptors (Inhibition Concentration (IC_50_) = 4.63–6.67 nM) versus σ_2_ receptors (1, 6). Small modifications in the SA4503 structure appear to have profound effects on the σ_1_/σ_2_ receptor affinity and selectivity (7). SA5403 has been labeled with ^11^C for PET studies of σ receptors in monkeys and humans (8-10). However, the equilibrium state of the receptor–ligand binding in monkeys could not be measured with [^11^C]SA4503 because of the short t_½_ of ^11^C. In an effort to overcome this problem, Elsinga et al. (7) synthesized [^18^F]fluoroethyl analog of SA45043 ([^18^F]FE-SA4503), which has a longer physical t_½_, so that the equilibrium state of receptor–ligand binding can be studied. However, [^18^F]FE-SA4503 is a non–subtype-selective σ receptor ligand. Kawamura et al. (1) synthesized [^18^F]FM-SA4503 as a selective σ_1_ receptor ligand.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5B18F%5DSA4503+OR+(fluorine-18-labeled+SA4503)+AND+synthesis)]

Fujimura et al. (11) reported the synthesis of SA4503 and other analogs of lefetamine. SA4503 was obtained by reacting N,N-bis(2-chloroethyl)-2-(3, 4-dimethoxy)phenylethylamine with phenylpropylamine. [^18^F]FM-SA4503 was synthesized by reacting 4-O-demethyl SA4503 with [^18^F]fluoromethyl bromide. 4-O-demethyl SA4503 was prepared from the starting material of 3-phenyl-1-propanol (11). Briefly, ^18^F-labeled fluoride was added to Kryptofix 2.2.2 in acetonitrile and heated at 130ºC. After cooling, methylene bromide was added and heated to reflux for 5 min. The resulting [^18^F]fluoromethyl bromide was added to a mixture of 4-O-demethyl SA4503 and sodium hydride in N,N-dimethylformamide. The reaction mixture was heated at 120ºC for 3 min and then acidified with hydrochloric acid and purified by high-performance liquid chromatography (HPLC). The radiochemical yield was 2.9–16.6% (n = 4) at the end of bombardment. The radiochemical purity was >99% with a specific activity of 37.8–283 TBq/mmol (1.02–7.6 Ci/μmol) at the end of synthesis (80 min at end of bombardment).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5B18F%5DSA4503+OR+(fluorine-18-labeled+SA4503)+AND+synthesis)]

The in vitro σ_1_ receptor binding affinity of unlabeled FM-SA4503 was studied in rat cerebral membranes with (+)-pentazocine (σ_1_ receptor ligand) as the competing ligand (1). In the σ_2_ receptor assay, rat liver membranes were used with 3-di(2-tolyl)guanidine. The selective affinities (K_i_) of FM-SA4503 were found to be 6.4 ± 1.3 nM (σ_1_ receptor) and 250 ± 16 nM (σ_2_ receptor).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5B18F%5DSA4503+OR+(fluorine-18-labeled+SA4503)+AND+synthesis)]

Biodistribution of [^18^F]FM-SA4503 was performed in mice with an i.v. dose of 0.22 MBq/5.8 pmol (5.9 μCi/5.8 pmol) (1). The brain activity increased for 30 min and then decreased. The brain radioactivity concentrations (percent injected dose per g (% ID/g); n = 4–5) were 3.15 ± 0.35, 3.39 ± 0.49, 4.30 ± 0.51, 3.87 ± 0.68, and 3.78 ± 0.52 at 5, 15, 30, 60, and 120 min, respectively. At 5 min, the radioactivity levels (% ID/g) for the major organs were 23.49 ± 3.73 (lung), 13.68 ± 2.35 (liver), 12.23 ± 1.49 (small intestine), 7.37 ± 1.33 (spleen), 6.92 ± 1.45 (pancreas), 4.32 ± 0.57 (heart), 2.09 ± 0.28 (bone), 0.93 ± 0.14 (blood), 1.89 ± 0.40 (muscle), and 4.90 ± 0.21 (kidney). At 60 min, these levels changed to 10.26 ± 1.08 (lung), 22.20 ± 3.65 (liver), 9.89 ± 1.39 (small intestine), 7.95 ± 1.34 (spleen), 10.68 ± 3.01 (pancreas), 1.61 ± 0.18 (heart), 2.50 ± 0.49 (bone), 0.25 ± 0.03 (blood), 1.11 ± 0.15 (muscle), and 8.30 ± 2.56 (kidney). Blocking studies with co-injection of 2 μmol/kg haloperidol (a σ_1_ and σ_2_ receptor ligand) or 2 μmol/kg unlabeled SA4503 showed that the brain radioactivity (n = 5) at 60 min was significantly decreased from 4.13 ± 0.34% ID/g (control) to 1.30 ± 0.10% ID/g and 2.14 ± 0.14% ID/g, respectively (1). The radioactivity levels in the heart, lung, liver, spleen, small intestine, and muscle were also decreased.

Metabolite studies in mice showed that 8.4 ± 1.2% (n = 3) of [^18^F]FE-SA4503 remained unchanged in the plasma at 60 min (1). In the brain, 94.1 ± 1.0% of the radioligand remained intact at 60 min.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((%5B18F%5DSA4503+OR+(fluorine-18-labeled+SA4503)+)+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5B18F%5DSA4503+OR+(fluorine-18-labeled+SA4503)+AND+synthesis)]

Kawamura et al. (1) studied the kinetics and metabolism of [^18^F]FM-SA4503 with PET imaging in two conscious rhesus monkeys. The monkey received an i.v. dose of 520 MBq/1.8 nmol (14.1 mCi/1.8 nmol) of [^18^F]FE-SA4503. After one week, PET imaging on the same monkey was also performed after pretreatment with haloperidol (1 mg/kg) and 480 MBq/2.2 nmol (13 mCi/2.2 nmol) [^18^F]FM-SA4503. A displacement study was performed in another monkey with a dose of 510 MBq/1.8 nmol (13.8 mCi/1.8 nmol) [^18^F]FM-SA4503. Haloperidol was administered 90 min after the radioligand injection. In the baseline study, the authors observed that [^18^F]FM-SA4503 was widely distributed throughout the brain in a pattern similar to [^11^C]SA4503. There were high radioactivity levels in several cortical areas, the thalamus, striatum, and cerebellum. The brain radioactivity level gradually increased over 120 min after injection, followed by a stable plateau phase until 180 min. The authors suggested that the receptor–ligand binding reached equilibrium after 120 min. Haloperidol pretreatment decreased the radioactivity levels to 22–32%, 17–29%, and 16–25% of the baseline at 60, 80, and 180 min, respectively. Similar effects were observed with the displacement study.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(%5B18F%5DSA4503+OR+(fluorine-18-labeled+SA4503))+AND+human)]

No publication is currently available.

## References

1 Kawamura K., Tsukada H., Shiba K., Tsuji C., Harada N., Kimura Y., Ishiwata K. (2007). Synthesis and evaluation of fluorine-18-labeled SA4503 as a selective sigma(1) receptor ligand for positron emission tomography. Nucl Med Biol.
2 Lever J.R., Gustafson J.L., Xu R., Allmon R.L., Lever S.Z. (2006). Sigma1 and sigma2 receptor binding affinity and selectivity of SA4503 and fluoroethyl SA4503. Synapse.
3 Skuza G., Wedzony K. (2004). Behavioral pharmacology of sigma-ligands. Pharmacopsychiatry.
4 Skuza G. (2003). Potential antidepressant activity of sigma ligands. Pol J Pharmacol.
5 Ishiguro H., Ohtsuki T., Toru M., Itokawa M., Aoki J., Shibuya H., Kurumaji A., Okubo Y., Iwawaki A., Ota K., Shimizu H., Hamaguchi H., Arinami T. (1998). Association between polymorphisms in the type 1 sigma receptor gene and schizophrenia. Neurosci Lett.
6 Matsuno K., Nakazawa M., Okamoto K., Kawashima Y., Mita S. (1996). Binding properties of SA4503, a novel and selective sigma 1 receptor agonist. Eur J Pharmacol.
7 Elsinga P.H., Kawamura K., Kobayashi T., Tsukada H., Senda M., Vaalburg W., Ishiwata K. (2002). Synthesis and evaluation of [18F]fluoroethyl SA4503 as a PET ligand for the sigma receptor. Synapse.
8 Kawamura K., Kubota K., Kobayashi T., Elsinga P.H., Ono M., Maeda M., Ishiwata K. (2005). Evaluation of [11C]SA5845 and [11C]SA4503 for imaging of sigma receptors in tumors by animal PET. Ann Nucl Med.
9 Kawamura K., Ishiwata K., Tajima H., Ishii S., Matsuno K., Homma Y., Senda M. (2000). In vivo evaluation of [(11)C]SA4503 as a PET ligand for mapping CNS sigma(1) receptors. Nucl Med Biol.
10 van Waarde A., Buursma A.R., Hospers G.A., Kawamura K., Kobayashi T., Ishii K., Oda K., Ishiwata K., Vaalburg W., Elsinga P.H. (2004). Tumor imaging with 2 sigma-receptor ligands, 18F-FE-SA5845 and 11C-SA4503: a feasibility study. J Nucl Med.
11 Fujimura K., Matsumoto J., Niwa M., Kobayashi T., Kawashima Y., In Y., Ishida T. (1997). Synthesis, structure and quantitative structure-activity relationships of sigma receptor ligands, 1-[2-(3,4-dimethoxyphenyl)ethyl]-4-(3-phenylpropyl) piperazines. Bioorg Med Chem.